# ^66^Ga-Labeled NOTA-conjugated anti-CD105 (endoglin) chimeric monoclonal antibody

Chemical name: | ^66^Ga-Labeled NOTA-conjugated anti-CD105 (endoglin) chimeric monoclonal antibody
Abbreviated name: | [^66^Ga]-NOTA-TRC105
Synonym:
Agent Category: | Antibody
Target: | CD105 (endoglin) antigen
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^66^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=CD105&cmd=DetailsSearch)]

The CD105 antigen (endoglin) is a hypoxia-inducible, 180-kDa, disulfide-linked homodimeric transmembrane glycoprotein that is a co-receptor for the transforming growth factor β (TGF-β) (1). Both CD105 and TGF-β are expressed at low levels in resting endothelial cells, but they are overexpressed in cancerous lesions and play a significantly proangiogenic role in remodeling the vasculature of malignant tumors (2). It has been shown that the levels of CD105 in endothelial tissues correlate well with the degree of cell proliferation, and that the antigen is a suitable biomarker to quantify tumor angiogenesis and can be used to determine the prognostic outcome for cancer patients (3). Investigators have reported that immunotoxins and radioimmunoconjugates generated with anti-CD105 monoclonal antibodies (mAbs) can inhibit angiogenesis and prevent the growth and metastasis of cancerous tumors (4). The biological activity of CD105 has been discussed in detail by Seon et al. (4). For translation to the clinic, a human/mouse chimeric anti-CD105 mAb (designated c-SNj6 or TRC105) has been generated and shown to have suitable pharmacokinetic, toxicological, and immunogenicity characteristics for use in non-human primates (5). Currently, a clinical trial (http://clinicaltrials.gov/ct2/show/NCT01326481?term=endoglin&rank=5) is in progress to evaluate the use of TRC105 for the treatment of metastatic breast cancer.

TRC105 has been labeled with ^64^Cu (6) and ^89^Zr (7), respectively, and shown to detect the expression of CD105 with positron emission tomography (PET) imaging in xenograft tumors in mice. In another study, TRC105 was conjugated to IRDye 800CW, a near-infrared fluorescent (NIRF) dye, and the expression of CD105 in tumors was visualized with NIRF imaging (8). TRC105 has been conjugated with ^64^Cu and IRDye 800CW to develop a dual-modality (PET/NIRF) imaging agent that has been used to detect murine breast cancer 4T1 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology) cell tumors in mice (9). Recently it has become possible to produce ^66^Ga (t_1/2_ = 9.3 h, E_0_ = 4.15 MeV), which has a very high specific activity and reacts with 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA), a bifunctional chelating agent, to yield a product ([^66^Ga]-NOTA) that has a specific activity of >70 GBq/μmol (>2 Ci/μmol), a value that is several-fold higher than those published in the literature (<4.6 GBq/μmol (~125 mCi/μmol)) (10). The investigators suggested that the high specific activity of the NOTA-conjugated radionuclide could be utilized to label peptides and biomolecules such as proteins and mAbs for PET imaging. In an ongoing effort to develop an immuno-PET agent that would be suitable for the noninvasive imaging of angiogenesis in tumor, TRC105 was conjugated with NOTA, labeled with ^66^Ga ([^66^Ga]-NOTA-TRC105), and evaluated for the PET visualization of CD105 expression in 4T1 cell tumors in mice (11).

### Related Resource Links

TRC105 (http://www.ncbi.nlm.nih.gov/books/?term=TRC105+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) chapters in MICAD

Other anti-CD105 antibody chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-CD105+antibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human CD105 (endoglin) protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/BC014271.2) sequences

CD105 gene information (http://www.ncbi.nlm.nih.gov/gene/2022) (Gene ID: 2022)

CD105 in Online Mendelian Inheritance in Man Database (http://omim.org/entry/131195) (OMIM)

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=TRC105) related to TRC105

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-TRC105%20synthesis&cmd=DetailsSearch)]

The ^66^Ga preparation used to perform this work was reported to contain <2 ppb nonradioactive Ga and <20 ppb Fe as determined with inductively coupled plasma mass spectroscopy (11).

TRC105 was obtained from a commercial source and conjugated with NOTA as described by Engle et al. (11). On average, ~5 NOTA molecules were conjugated to each of the mAbs as determined with ultraviolet spectrophotometric analysis (9). NOTA-TRC105 was labeled with ^66^Ga and purified with size-exclusion chromatography using phosphate-buffered saline containing 0.25 M ammonium acetate (pH 7.2) as the mobile phase (11). The final radioimmunoconjugate preparation was passed through a 0.22-μm filter for use in in vivo studies.

Cetuximab (a human/mouse chimeric mAb that targets the human epidermal growth factor receptor) was obtained from a pharmaceutical company and used to prepare [^66^Ga]-NOTA-cetuximab as described above (11). ^66^Ga-Labeled cetuximab was used as a control in some studies.

The total time to prepare the two purified ^66^Ga-labeled mAbs was reported to be 70 ± 10 min (n = 7 preparations), and both labeled mAbs had a radiochemical yield and radiochemical purity of 80.2 ± 4.1% and >95%, respectively (11). The specific activity of the two ^66^Ga-labeled mAbs was ~1.2 GBq (32.4 mCi)/6.6 nmol.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-TRC105%20in%20vitro&cmd=DetailsSearch)]

A fluorescence-assisted cell-sorting analysis of HUVEC (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1730&Template=cellBiology) cells (human umbilical vein endothelial cells that have a high expression of CD105) and MCF-7 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-22&Template=cellBiology) cells (human breast mammary gland cells that do not express CD105) showed that both TRC105 and NOTA-TRC105 had similar affinities for the CD105 antigen on the HUVEC cells (11). Neither TRC105 nor NOTA-TRC105 showed any binding to the MCF-7 cells. This indicated that the conjugation of NOTA to TRC105 did not alter its affinity or specificity for the CD105 antigen expressed on the HUVEC cell surface (11). No blocking studies were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-TRC105%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^66^Ga]-NOTA-TRC105 was investigated in mice bearing murine breast cancer 4T1 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology) cell tumors as described by Engle at al (11). The animals (n = 4 mice) were given an intravenous injection of the tracer and euthanized at 36 h postinjection (p.i.) to retrieve all the major organs, including the tumors, to determine the amount of radioactivity accumulated in the various tissues. Data obtained from the study were presented as percent of injected dose per gram tissue (% ID/g). Maximum radioactivity was detected in the blood (~12.5% ID/g), followed by the tumors (~10% ID/g), lungs (~6% ID/g), and the liver, kidney, and spleen (each of these organs showed an accumulation of ~5% ID/g). All other organs had an uptake of <2.5% ID/g. The tumor/muscle uptake ratio (T/M ratio) was calculated to be 10.1 ± 1.1 at 36 h p.i. When the mice (n = 4 animals) were given a blocking dose of TRC105 (13.3 nmol) 2 h before injecting the radioimmunoconjugate, the T/M ratio decreased significantly (~6.0; P < 0.01), and a simultaneous increase in accumulation of label was observed in the liver and lungs. Pretreatment of the mice with escalating doses of NOTA-TRC105 (ranging from 3.33 pmol to 666 pmol) did not change the amount of radioactivity accumulated in the tumors (8.8 ± 1.2% ID/g, 9.9 ± 1.2% ID/g, 8.5 ± 0.5% ID/g, and 8.0 ± 0.5% ID/g at 3.33, 16.65, 83.5, and 666 pmol NOTA-TRC105, respectively). These studies indicated that [^66^Ga]-NOTA-TRC105 had a binding specificity for the CD105 antigen.

The uptake of [^66^Ga]-NOTA-TRC105 was compared to that of [^66^Ga]-NOTA-cetuximab in the different tissues of mice bearing 4T1 cell tumors (n = 4 mice/group) (11). Except for the liver and the tumors, all other tissues from the animals showed a similar uptake of radioactivity from both ^66^Ga-labeled mAbs. The tumors showed a significantly higher (P < 0.01) uptake of label with ^66^Ga-NOTA-TRC105 (~10% ID/g) than with ^66^Ga-NOTA-cetuximab (~3.5% ID/g). However, the liver showed higher accumulation of the tracer with ^66^Ga-NOTA-cetuximab (~6.0% ID/g) than with ^66^Ga-NOTA-TRC105 (~4.0% ID/g). This suggested that the CD105 antigen was targeted specifically by the ^66^Ga-labeled TRC105 mAb.

For PET imaging of mice bearing 4T1 cell tumors (n = 4 animals), the rodents were given an intravenous injection of [^66^Ga]-NOTA-TRC105 (dose not mentioned), and whole-body images of the animals were acquired at 4, 20, and 36 h p.i (11). Quantitative data were obtained from the images with region-of-interest analysis as described by Engle et al. (11). The initial time point (4 h p.i.) showed a high level of radioactivity in the blood pool, and this level decreased gradually at the subsequent time points. The tumors were visible at 4 h p.i. and had an uptake of 5.9 ± 1.6% ID/g. The amount of tracer in these lesions increased to 8.5 ± 0.6 at 20 h p.i. and remained constant thereafter (9.0 ± 0.6% ID/g at 36 h p.i.). The liver showed a decrease in accumulation of radioactivity over time (10.6 ± 1.8% ID/g, 8.2 ± 0.4% ID/g, and 6.8 ± 0.5% ID/g at 4, 20, and 36 h p.i. respectively); however, the blood showed a relatively constant level of the tracer at all the time points (10.3 ± 1.9% ID/g, 9.4 ± 0.9% ID/g, and 9.0 ± 0.6% ID/g at 4, 20, and 36 h p.i. respectively). To determine the in vivo target-binding specificity of [^66^Ga]-NOTA-TRC105, the animals (n = 4 mice) were injected with 13.3 nmol nonradioactive TRC105 2 h before administration of the ^66^Ga-labeled TRC105 (11). PET images of the animals were acquired as before. The uptake of label in the tumors was 4.4 ± 1.2% ID/g, 5.8 ± 0.6% ID/g, and 7.2 ± 0.6% ID/g at 4, 20, and 36 h p.i., respectively, which was significantly lower (P < 0.05 at 20 h p.i. and 36 h p.i.) than the accumulation observed in the lesions of animals injected with [^66^Ga]-NOTA-TRC105 alone (for uptake values, see above). The accumulation of radioactivity in the blood and liver of animals given the blocking dose was similar to that of animals injected with [^66^Ga]-NOTA-TRC105 alone at all the time points. Therefore, this study confirmed the in vivo CD105 binding specificity of the radioimmunoconjugate.

To further confirm the in vivo specificity of [^66^Ga]-NOTA-TRC105, isotype-matched [^66^Ga]-NOTA-cetuximab was injected as a control in mice bearing 4T1 cell tumors (n = 4 animals), and PET images were acquired from the animals at the same time points mentioned above (11). From the images, it was calculated that the amount of label in the tumors was 2.7 ± 0.5% ID/g, 4.2 ± 1.2% ID/g, and 4.1 ± 0.8% ID/g at 4, 20, and 36 h p.i., respectively, which was significantly lower than the accumulation of tracer observed with [^66^Ga]-NOTA-TRC105 at all examined time points (P < 0.05 at 4 h p.i.; P < 0.01 at 20 h p.i. and 36 h p.i.). Results from this study showed that [^66^Ga]-NOTA-TRC105 bound specifically to the CD105 antigen.

From these studies, the investigators concluded that [^66^Ga]-NOTA-TRC105 is a suitable agent to detect tumors that expressed the CD105 antigen in rodents (11).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-TRC105%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-TRC105%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-TRC105%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

This work was supported in part by grant 9U54TR000021 from the National Center for Advancing Translational Sciences (NCATS) and the National Institutes of Health through the UW Radiological Sciences Training Program 5 T32 CA009206-32.

## References

1 Nassiri F., Cusimano M.D., Scheithauer B.W., Rotondo F., Fazio A., Yousef G.M., Syro L.V., Kovacs K., Lloyd R.V. (2011). Endoglin (CD105): a review of its role in angiogenesis and tumor diagnosis, progression and therapy. Anticancer Res.
2 Perez-Gomez E., Del Castillo G., Juan Francisco S., Lopez-Novoa J.M., Bernabeu C., Quintanilla M. (2010). The role of the TGF-beta coreceptor endoglin in cancer. ScientificWorldJournal.
3 Fonsatti E., Nicolay H.J., Altomonte M., Covre A., Maio M. (2010). Targeting cancer vasculature via endoglin/CD105: a novel antibody-based diagnostic and therapeutic strategy in solid tumours. Cardiovasc Res.
4 Seon B.K., Haba A., Matsuno F., Takahashi N., Tsujie M., She X., Harada N., Uneda S., Tsujie T., Toi H., Tsai H., Haruta Y. (2011). Endoglin-targeted cancer therapy. Curr Drug Deliv.
5 Shiozaki K., Harada N., Greco W.R., Haba A., Uneda S., Tsai H., Seon B.K. (2006). Antiangiogenic chimeric anti-endoglin (CD105) antibody: pharmacokinetics and immunogenicity in nonhuman primates and effects of doxorubicin. Cancer Immunol Immunother.
6 Hong H., Yang Y., Zhang Y., Engle J.W., Barnhart T.E., Nickles R.J., Leigh B.R., Cai W. (2011). Positron emission tomography imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
7 Hong H., Severin G.W., Yang Y., Engle J.W., Zhang Y., Barnhart T.E., Liu G., Leigh B.R., Nickles R.J., Cai W. (2012). Positron emission tomography imaging of CD105 expression with 89Zr-Df-TRC105. Eur J Nucl Med Mol Imaging.
8 Yang Y., Zhang Y., Hong H., Liu G., Leigh B.R., Cai W. (2011). In vivo near-infrared fluorescence imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
9 Zhang Y., Hong H., Engle J.W., Yang Y., Theuer C.P., Barnhart T.E., Cai W. (2012). Positron Emission Tomography and Optical Imaging of Tumor CD105 Expression with a Dual-Labeled Monoclonal Antibody. Mol Pharm.
10 Engle, J.W., V. Lopez-Rodriguez, R.E. Gaspar-Carcamo, H.F. Valdovinos, M. Valle-Gonzalez, F. Trejo-Ballado, G.W. Severin, T.E. Barnhart, R.J. Nickles, and M.A. Avila-Rodriguez, Very high specific activity (66/68)Ga from zinc targets for PET. Appl Radiat Isot, 2012
11 Engle J.W., Hong H., Zhang Y., Valdovinos H.F., Myklejord D.V., Barnhart T.E., Theuer C.P., Nickles R.J., Cai W. (2012). Positron emission tomography imaging of tumor angiogenesis with a (66)Ga-labeled monoclonal antibody. Mol Pharm.